# ^18^F-Labeled N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-[^18^F]-fluoroethoxy)-5-iodo-3-methoxybenzamide

Chemical name: | ^18^F-Labeled N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-[^18^F]-fluoroethoxy)-5-iodo-3-methoxybenzamide | [image]
Abbreviated name: | [^18^F]3f | [image]
Synonym: | | [image]
Agent Category: | Compound | [image]
Target: | Sigma-2 receptor | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]3f.

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/pubmed?term=sigma%202%20receptor&cmd=DetailsSearch)

Sigma receptor (SR) subtypes 1 (Sig-1R) and 2 (Sig-2R) and are known to be present primarily in the central nervous system and the peripheral tissues. Both receptor subtypes have a different distribution in the two types of tissues, and the exact biological function of these receptors is not known (1). Of the two receptor subtypes, only the Sig-1R has been cloned, expressed, and purified (2). The Sig-2R is known to be overexpressed in various malignant tumors and is believed to promote cell proliferation, indicating that these receptors may play a role in the development of some cancers (3). As a consequence the Sig-2R have been suggested to be biomarkers for tumor cell proliferation (4) and could be targeted for the development of different anti-cancer drugs (5) or imaging agents for tumors that overexpress Sig-2R (3, 5). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=sigma+2+receptor) have been approved by the United States Food and Drug Administration for the evaluation of drugs that target the Sig-2R for the imaging and treatment of different clinical conditions. In addition, Sig-2R ligands have been used in preclinical studies to chemosensitize (http://mct.aacrjournals.org/content/2/8/805.full.pdf+html) tumors to low doses of anti-cancer drugs that are otherwise toxic when given at high doses to animals bearing mammalian cell line tumors (6, 7).

Investigators have developed and characterized several SR ligands, but most of them are either selective only for the Sig-1R or have similar affinity for both the SR subtypes, therefore limiting their use as anti-cancer drugs that target the Sig-2R or as detection and imaging agents for this receptor (3, 7). In an effort to develop a ligand with high specificity for Sig-2R, Tu et al. synthesized a series of ^18^F-labeled benzamide analogs and evaluated these radiolabeled compounds with positron emission tomography (PET) and computed tomography (CT) imaging of mice bearing allograft tumors expressing the receptor (3). Among the various compounds tested, N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-[^18^F]-fluoroethoxy)-5-iodo-3-methoxybenzamide (designated [^18^F]3f) and another analog, N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-[^18^F]-fluoroethoxy)-5-methylbenzamide (designated [^18^F]3c), were determined to be most suitable for the detection of solid tumors expressing Sig-2R with the use of PET and CT imaging. This chapter describes the in vitro characterization and in vivo biodistribution of [^18^F]3f and the PET/CT imaging with [^18^F]3f. The in vitro and in vivo characterization of [^18^F]3c are described in a separate chapter in MICAD (www.micad.nih.gov) (8).

### Other sources of information regarding SRs

Other SR imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=sigma+receptor++AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

Sigma receptors in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=sigma%20receptors) (Online Mendelian Inheritance in Man).

Protein sequences of human SR1, isoform1 (http://www.ncbi.nlm.nih.gov/protein/NP_005857.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and isoform 2 (http://www.ncbi.nlm.nih.gov/protein/NP_671513.1?ordinalpos=2&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum).

Nucleotide (mRNA) sequences of SR1, variant 1 (http://www.ncbi.nlm.nih.gov/nuccore/NM_005866.2?ordinalpos=4&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and variant 2 (http://www.ncbi.nlm.nih.gov/nuccore/NM_147157.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%5BAll%20Fields%5D%20AND%20%28%22metabolism%22%5BMeSH%20Terms%5D%20OR%20%22metabolism%22%5BAll%20Fields%5D%20OR%20%22synthesis%22%5BAll%20Fields%5D%29&cmd=DetailsSearch&log$=details)]

The synthesis and ^18^F-labeling of 3f has been described by Tu et al. (3). The total time of synthesis to obtain [^18^F]3f was ~2 h with a decay-corrected yield of ~30%. The radiochemical purity of the labeled compound was >99% as determined with analytical high-performance liquid chromatography with a specific activity of >74.07 TBq/mmol (2,000 Ci/mmol). The stability and conditions used to store [^18^F]3f were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20in%20vitro&cmd=DetailsSearch)]

In vitro receptor binding studies with [^18^F]3c were performed by Tu et al. (3) using membranes isolated from liver homogenates as described elsewhere (9). The affinity of 3c for the two SR subtypes was determined by competition studies using [^3^H](+)-pentazocine (for Sig-1R) and [^3^H]1,3-di(2-tolyl)guanidine in the presence of unlabeled (+)-pentazocine (for Sig-2R). The affinity of 3f, as determined with Scatchard plot analysis, was reported to be 2,150 ± 410 and 0.26 ± 0.07 nM for Sig-1R and Sig-2R, respectively, with a Sig-1R/Sig-2R ratio of 8,190. For comparison, the affinity of 3c was reported to be 330 ± 25 and 6.95± 1.63 nM, respectively, for the two receptor subtypes, with a Sig-1R/Sig-2R ratio of 48.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20rodentia&cmd=DetailsSearch)]

Tu et al. studied the biodistribution of [^18^F]3f in BALB/c mice bearing mouse mammary adenocarcinoma EMT-6 cell (these cells express high levels of both SR subtypes (10)) tumors (3). The animals were injected with the labeled compound through the tail vein and euthanized at predetermined time points up to 120 min after the treatment (the number of animals used per time point was not indicated). After euthanasia, tissues from major organs of the animals were removed, weighed, and counted for accumulated radioactivity, and the data were presented as a percentage of injected dose per gram tissue (% ID/g). At 5 min after injection, maximum uptake of radioactivity was noticed in the kidneys (19.98 ± 1.66% ID/g) followed by the liver (15.12 ± 2.21% ID/g) and lungs (18.47 ± 3.07% ID/g). In comparison, the tumor had an uptake of 3.05 ± 0.43% ID/g at this time point. By 2 h after injection, the amount of label in the kidney, liver, lungs, and tumor tissues was reduced to 1.34 ± 0.10, 2.61 ± 0.69, 0.74 ± 0.03, and 1.15 ± 0.23% ID/g, respectively. A similar trend was noticed for the uptake of [^18^F]3f in all the tissues, including the tumors. The tumor/muscle (T/M) and tumor/fat (T/F) ratios for [^18^F]3f were ~7 and ~6, respectively, at 2 h after injection. For [^18^F]3c, the T/M and T/F ratios were ~3 and ~8, respectively. Both [^18^F]3f and [^18^F]3c were reported to have rapid clearance from blood, indicating that both tracers were probably suitable for the detection and imaging of solid tumors expressing Sig-2R.

For blocking studies, mice were injected with [^18^F]3f in the presence of excess (1 mg/Kg) unlabeled N-(4-fluorobenzyl)piperidinyl-4-(3-bromophenyl) acetamide, which has a high affinity for the SR (3), and the mice were euthanized 1 h after the treatment (the number of animals used was not reported) (3). Under these conditions, the T/M and T/F ratios for this labeled compound were reduced by ~50%, indicating that the radiochemical bound selectively to the Sig-2R. Similar results were obtained with [^18^F]3c under these experimental conditions.

Mice bearing EMT-6 cell tumors were injected with [^18^F]3f as detailed above, and PET/CT imaging was performed on the animals 1 h later (3). Both detection methods were reported to identify the tumors in the animals easily. Similar results were reported when [^18^F]3c was used as an imaging agent.

On the basis of results obtained from these studies, the investigators concluded that both [^18^F]3f and [^18^F]3c were equally suitable for the detection and imaging of solid tumors expressing Sig-2R using PET (3).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-3c%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Some studies reported in this chapter were supported by National Institutes of Health grants CA-102869 and P41RR0954.

## References

1 Collier T.L., Waterhouse R.N., Kassiou M. (2007). Imaging sigma receptors: applications in drug development. Curr Pharm Des.
2 Hanner M., Moebius F.F., Flandorfer A., Knaus H.G., Striessnig J., Kempner E., Glossmann H. (1996). Purification, molecular cloning, and expression of the mammalian sigma1-binding site. Proc Natl Acad Sci U S A.
3 Tu Z., Xu J., Jones L.A., Li S., Dumstorff C., Vangveravong S., Chen D.L., Wheeler K.T., Welch M.J., Mach R.H. (2007). Fluorine-18-labeled benzamide analogues for imaging the sigma2 receptor status of solid tumors with positron emission tomography. J Med Chem.
4 Wheeler K.T., Wang L.M., Wallen C.A., Childers S.R., Cline J.M., Keng P.C., Mach R.H. (2000). Sigma-2 receptors as a biomarker of proliferation in solid tumours. Br J Cancer.
5 Hashimoto K., Ishiwata K. (2006). Sigma receptor ligands: possible application as therapeutic drugs and as radiopharmaceuticals. Curr Pharm Des.
6 Kashiwagi H., McDunn J.E., Simon P.O., Goedegebuure P.S., Vangveravong S., Chang K., Hotchkiss R.S., Mach R.H., Hawkins W.G. (2009). Sigma-2 receptor ligands potentiate conventional chemotherapies and improve survival in models of pancreatic adenocarcinoma. J Transl Med.
7 Chu W., Xu J., Zhou D., Zhang F., Jones L.A., Wheeler K.T., Mach R.H. (2009). New N-substituted 9-azabicyclo[3.3.1]nonan-3alpha-yl phenylcarbamate analogs as sigma2 receptor ligands: synthesis, in vitro characterization, and evaluation as PET imaging and chemosensitization agents. Bioorg Med Chem.
8 Chopra, A., [18F]Labeled N-(4-(6,7-dimethoxy-3,4-dihydroisoquinolin-2(1H)-yl)butyl)-2-(2-[18F]-fluoroethoxy)-5-methylbenzamide ([18F]3c). Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
9 Xu J., Tu Z., Jones L.A., Vangveravong S., Wheeler K.T., Mach R.H. (2005). [3H]N-[4-(3,4-dihydro-6,7-dimethoxyisoquinolin-2(1H)-yl)butyl]-2-methoxy-5 -methylbenzamide: a novel sigma-2 receptor probe. Eur J Pharmacol.
10 Colabufo N.A., Berardi F., Contino M., Fazio F., Matarrese M., Moresco R.M., Niso M., Perrone R., Tortorella V. (2005). Distribution of sigma receptors in EMT-6 cells: preliminary biological evaluation of PB167 and potential for in-vivo PET. J Pharm Pharmacol.